# ^99m^Tc-Labeled anti-carcinoembryonic antigen monoclonal antibody CL-58

Chemical name: | ^99m^Tc-Labeled anti-carcinoembryonic antigen monoclonal antibody CL-58
Abbreviated name: | ^99m^Tc-Anti-CEA CL-58
Synonym: | ^99m^Tc-CL-58
Agent Category: | Monoclonal antibody
Target: | Carcinoembryonic antigen (CEA)
Target Category: | Antibody-ligand binding
Method of detection: | Single-photon emission computed tomography; planar gamma imaging
Source of Signal/Contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click here for protein and nucleotide (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=634&log$=databasead&logdbfrom=protein) information regarding carcinoembryonic antigen

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D)]

The occurrence of colon and rectal cancer is influenced by genetic, nutritional, environmental, and occupational factors (1). Surgical removal of rectal cancer is considered to be the most common treatment for this ailment, and the additional use of chemotherapy and/or radiotherapy is known to improve treatment outcomes (2). However, in spite of the available treatments, recurrence and metastasis of the cancer primarily determine the success of long-term care and quality of life for these cancer patients (3, 4). Early detection of the cancer and its recurrence or metastasis could help devise a suitable treatment regimen and prolong patient survival with a suitable quality of life. After treatment, the patients usually undergo periodic computed tomography (CT) scans or fibrocolonoscopy as well as invasive procedures such as ultrasonography or CT-guided needle biopsy to monitor for any recurrence of the disease, but these procedures do not always detect recurrent disease lesions (5).

Carcinoembryonic antigen (CEA) is a tumor-associated antigen that is secreted into the serum of rectal cancer patients, and its level is monitored after treatment to detect possible recurrence of the cancer. Although these tests have a high specificity, they lack the sensitivity to accurately detect disease recurrence (6, 7). To improve the sensitivity of the test to detect CEA for radioimmunoguided surgical treatment of the cancer, investigators developed the monoclonal antibody (MAb) CL-58, which is directed against the CEA, and they radiolabeled it with radioactive iodine (^125^I) and used it to identify micrometastasis in patients (8). In another study, CL-58 was labeled with radioactive technetium (^99m^Tc), and its biodistribution was studied in nude mice bearing human xenograft tumors (8). The labeled MAb was also evaluated for the detection of recurrent rectal cancer in humans (5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+CL58+synthesis)]

The CL-58 MAb was generated as described by Yao et al. (5). Briefly, Balb/c mice were immunized with human CEA, and spleen cells obtained from these animals were fused with mouse SP2/0-Ag14 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1581&Template=cellBiology) melanoma cells to generate hybridomas that were grown in mouse ascites. The CL-58 MAb was purified with column chromatography using protein A affinity and high-performance hydroxylapatite columns. Purity of the MAb was >95% as determined with sodium dodecyl sulphate polyacrylamide gel electrophoresis.

To label CL-58 with ^99m^Tc, the MAb was reduced with 2-mercaptoethanol and purified on a PD-10 column (5). The reduced MAb was mixed with an equal amount of glucoheptonate, and freshly prepared stannous chloride was added to the mixture. Sodium [^99m^Tc]pertechnetate was subsequently added to the mixture and incubated for 15 min at room temperature before the labeling efficiency of the reaction was tested (method was not specified). The conjugation rate was reported to be >90%, and <2% free ^99m^Tc was detected. If the labeling efficiency was <90%, the labeled MAb was purified on a PD-10 column before use. Usually the labeled MAb was not purified after labeling, and or sterilized by filtration before clinical use (5). The stability and specific activity of the ^99m^Tc-labeled CL-58 were not reported in this study.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+MAb+CL58+in+vitrohttp://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

The affinity constant of CL-58 was reported to be 7.4 × 10^9^ L/mol as determined with a competition enzyme-linked immunosorbent assay (5). The MAb was reported to bind human CL-187 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CL-187&Template=cellBiology), HT-29 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-38&Template=cellBiology), and B-80 cells (see Toouli et al. (9) for characteristics of the B-80 cells) with high affinity, but it did not exhibit any binding to red blood, fibroblast, or bone marrow cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+MAb+CL58+rodentiahttp://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

The biodistribution of ^99m^Tc-labeled CL-58 was investigated in athymic mice (n = 5 animals) bearing xenograft CL-187 colon cancer cell tumors on the axilla (8). When the tumors reached a diameter of 15–35 mm^3^, the animals were injected with the [^99m^Tc]-anti-CEA CL-58 MAb and imaged with a gamma camera after 24 h. The animals were then killed, and the various organs were removed. The incorporated radioactivity was reported as % injected dose/gram of tissue (% ID/g), and the tumor:non-tumor (T:NT) ratios were calculated. The tumors had radioactive accumulation of 15 ± 2.75% ID/g, and the T:NT ratios for blood, kidneys, and the liver were 1.82, 1.52, and 2.92, respectively; the T:NT ratio for other organs was reported to be >3. The tumors on the axilla of the animals could be easily distinguished from other organs with gamma imaging, indicating that the labeled MAb accumulated specifically at the CEA-producing tumor (8). Competition studies using the unlabeled CL-58 MAb were not reported and as a result specificity of the MAb was not determined in this study.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+anti+CEA+CL58+non+primate+mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+anti+CEA+CL58+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

Yao et al. used immunoscintigraphy to evaluate the use of [^99m^Tc]-anti-CEA CL-58 for the detection of suspected recurrent rectal cancer in 36 patients (5). Among these patients, scintigraphy detected cancer in 31 individuals, and these findings were confirmed with endoscopy and a pathological examination. Five patients did not show any specific accumulation of radioactivity and had no pathological evidence of the disease. The scintigraphic detection of cancer with [^99m^Tc]-anti-CEA CL-58 was reported to have a positive detection rate of 86.11%, a specificity of 83.33%, and a sensitivity of 100%. No competition studies were reported. Also, among the 31 positive patients, 29 individuals had elevated CEA levels.

## Supplemental Information

[Disclaimers]

## References

1 Roemer H.C., Weistenhofer W., Lohlein D., Geller F., Blomeke B., Golka K. (2008). N-acetyltransferase 1 in colon and rectal cancer cases from an industrialized area. J Toxicol Environ Health A.
2 Lim S.B., Choi H.S., Jeong S.Y., Kim D.Y., Jung K.H., Hong Y.S., Chang H.J., Park J.G. (2008). Optimal surgery time after preoperative chemoradiotherapy for locally advanced rectal cancers. Ann Surg.
3 Bakx R., Sprangers M.A., Oort F.J., van Tets W.F., Bemelman W.A., Slors J.F., van Lanschot J.J. (2005). Development and validation of a colorectal functional outcome questionnaire. Int J Colorectal Dis.
4 Bakx R., van Tinteren H., van Lanschot J.J., Zoetmulder F.A. (2004). Surgical treatment of locally recurrent rectal cancer. Eur J Surg Oncol.
5 Yao Y.F., Yang Z., Li Z.F., Gu J. (2008). Immunoscintigraphy of local recurrent rectal cancer with 99mTc-labeled anti-CEA monoclonal antibody CL58. World J Gastroenterol.
6 Tan E., Gouvas N., Nicholls R.J., Ziprin P., Xynos E., Tekkis P.P. (2008). Diagnostic precision of carcinoembryonic antigen in the detection of recurrence of colorectal cancer. Surg Oncol.
7 Park J.Y., Lee K.H. (2007). Carcinoembryonic antigen and patterns of recurrence after curative resection of the colorectal cancer. Hepatogastroenterology.
8 Gu J., Zhao J., Li Z., Yang Z., Zhang J., Gao Z., Wang Y., Xu G. (2003). Clinical application of radioimmunoguided surgery in colorectal cancer using 125I-labeled carcinoembryonic antigen-specific monoclonal antibody submucosally. Dis Colon Rectum.
9 Toouli C.D., Huschtscha L.I., Neumann A.A., Noble J.R., Colgin L.M., Hukku B., Reddel R.R. (2002). Comparison of human mammary epithelial cells immortalized by simian virus 40 T-Antigen or by the telomerase catalytic subunit. Oncogene.